# 2-[^18^F]Fluoro-3-[2(S)-2-azetidinylmethoxy]pyridine

Chemical name: | 2-[^18^F]Fluoro-3-[2(S)-2-azetidinylmethoxy]pyridine
Abbreviated name: | 2-[^18^F]FA
Synonym: | 2-[^18^F]Fluoro-A-85380
Agent Category: | Compound
Target: | α4β2 nicotinic acetylcholine receptor (nAChR)
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-18F%20A-85380)]

Neuronal nicotinic cholinergic receptors (nAChRs) are a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine always causes a rapid increase in cellular permeability to ions, such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α (α2-α10) and four subtypes of structural β (β2-β5). nAChRs have been demonstrated to be involved in cognitive processes such as learning and memory and control of movement in normal subjects. Dysfunction of nAChR has been implicated to a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease (AD) and Parkinson's disease. nAChRs also play a significant role in nicotine addiction and related health problems associated with tobacco smoking.

3-[2(S)-2-azetidinylmethoxy]pyridine (A-85380) is a highly potent and selective α4β2 nAChR agonist with subnanomolar affinity (4). A-85380 has been labeled as 2-[^18^F]Fluoro-3-[2(S)-2-azetidinylmethoxy]pyridine (2-[^18^F]fluoro-A-85380) (5). 2-[^18^F]fluoro-A-85380 (2-[^18^F]FA) is being developed as a positron emission tomography (PET) agent for the non-invasive study of nAChR in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-18F%20A-85380%20and%20synthesis)]

Horti et al. (5) reported synthesis of 2-[^18^F]FA by a 2-step reaction, which consisted of standard ([^18^F]KF/Kryptofix 2.2.2) ^18^F-nucleophilic aromatic fluorination of 2-iodo-3-[2-((S)-N-tert-butoxycarbonyl-3-pyrroline)methoxy]pyridine and acidic deprotection of the product. An average radiochemical yield was 10% (end of synthesis, based on [^18^F]KF) with a total synthesis time of 120 min. The average specific activity was 39 GBq/μmol (1.05 Ci/μmol at end of synthesis) with a radiochemical purity of >99%.

Dolle et al. (6) improved the radiochemical yields of 2-[^18^F]FA by using 2-nitro-3-[2-((S)-N-tert-butoxycarbonyl-2-azetidinymethoxy]pyridine for ^18^F-nucleophilic aromatic fluorination with the total synthesis time of 50-53 min (end of bombardment). The average radiochemical yields were 49-52% with the specific activities of 111-185 GBq/μmol (3-5 Ci/μmol at end of synthesis) and radiochemical purity of >99%. Trimethylammonium trifluoromethanesulfonate could also be used as the leaving group for the ^18^F-nucleophilic aromatic substitution with similar results. Schmaljohann et al. (7) has automated the synthesis of 2-[^18^F]FA with 58% yield in 45 min using the trimethylammonium trifluoromethanesulfonate precursor with specific activity >55 GBq/μmol (>1.5 Ci/μmol) at end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-18F%20A-85380%20and%20in%20vitro)]

Sullivan et al. (4) reported that A-85380 had K_i_ values of 0.05 ± 0.01, 148 ± 13, and 314 ± 12 nM for human α4β2, α7, and muscle α1β1δγ receptors, respectively. A-85380 (up to 10,000 nM) has no effect in various neurotransmitter binding assays. Chefer et al. (8) determined that 2-[^18^F]FA had a K_d_ of 0.05 ± 0.003 nM and a B_max_ of 140 ± 5 fmol/mg protein in rat brain homogenates.

Schmaljohann et al. (7) performed in vitro autoradiography studies of rat brain slices indicated selective binding of 2-[^18^F]FA to thalamus >striatum>cortex >cerebellum, consistent with α4β2 receptor distribution. The ratios of specific binding to total binding in cerebellum were 3.58, 1.25, and 1.02 for the thalamus, striatum, and cortex, respectively. Nicotine (10 μM) blocked 2-[^18^F]FA specific binding across the brain regions. In postmortem human brain sections of AD (n = 2), there was a decrease in 2-[^18^F]FA binding in the thalamus (32-40%) and occipital cortex (15-57%) but not in the entorhinal cortex compared with the control brains (n = 2). In the control brain sections, the radioactivity in the thalamus was 1.5 times higher than the occipital cortex and entorhinal cortex.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-18F%20A-85380%20and%20rodentia)]

Horti et al. (5) performed biodistribution studies in mice after injection of 0.74-1.11 MBq (20-30 μCi) 2-[^18^F]FA (1 nmol/kg). A peak uptake of 1.86% injected dose (ID)/g was reached in the whole brain at 15 min, followed by a gradual washout to 0.19% ID/g at 180 min. 2-[^18^F]FA accumulation was higher in the thalamus (7.2% ID/g) and in superior colliculus (6.8% ID/g) and lower in the hippocampus (~1.8% ID/g) and cerebellum (~1.0% ID/g) at 30 min post injection. Nicotine or cytosine pretreatment significantly inhibited 2-[^18^F]FA binding in all regions of the brain, with marginal inhibition in the cerebellum. Scopolamine (a muscarinic AChR antagonist) did not exhibit any inhibition. Pretreatment with 2-fluoro-A-85380 (170 nmol/kg) blocked accumulation in the striatum, parietal cortex, thalamus and superior colliculus by 43, 75, 84, and 85%, respectively. Only marginal inhibition was observed in the cerebellum and hippocampus. Vaupel et al. (9) estimated binding potential (BP) values in the brain of rats with 2-[^18^F]FA PET imaging using free arterial plasma levels. The BP values for thalamus, forebrain, and cerebellum were 5.9 ± 0.7, 2.6 ± 0.4, and 1.0 ± 0.1, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-18F%20A-85380%20and%20%28dog%20or%20pig%20or%20cat%20or%20sheep%20or%20rabbit%29)

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-18F%20A-85380%20and%20%28primate%20not%20human%29)]

2-[^18^F]FA PET studies with non-human primates showed substantial brain accumulation with selective maximal uptake in the regions of the thalamus, intermediate uptake in the striatum and cortex (6, 8, 10). The cerebellum showed lower binding than the other brain regions. 2-[^18^F]FA radioactivity was blocked (pretreatment) and displaced by A-85380, nicotine and cytisine. Using graphical methods with arterial input function, Chefer et al. (11) estimated binding potential (BP) values of 2.0, 0.4, 0.3, and 0.03 observed in the thalamus, cortex, striatum, and cerebellum, respectively. For accurate quantization of [^18^F]FA specific binding by graphical analysis, PET studies should last up to 7 hours because of the slow kinetics of 2-[^18^F]FA brain distribution. The fraction of unchanged 2-[^18^F]FA in the plasma determined by HPLC was 50% at 60 min after injection. Two major hydrophilic metabolites were found.

Valette et al. (12) reported that physostigmine, a potent AChE inhibitor, inhibited the distribution volumes in the striatum, temporal cortex and frontal cortex (regions of interests) by 40, 23, and 30% in 2-[^18^F]FA PET studies in monkeys, respectively. The authors suggested that the effects of physostigmine may be the results of increased concentrations of synaptic acetylcholine, which could desensitize the nAChR and compete with 2-[^18^F]FA.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-18F%20A-85380%20and%20human)]

Human dosimetry of 2-[^18^F]FA was estimated in six normal volunteers ( three males and three females) by Kimes et al. (13). Dynamic whole-body PET scans were acquired after the injection of 1.6 ± 0.07 MBq/kg (0.043 ± 0.002 mCi/kg, 5 ± 2 pmol/kg) of 2-[^18^F]FA. There were no reported pharmacological effects associated with the 2-[^18^F]FA administrations. Uptake of 2-[^18^F]FA in the brain reached a peak of 2.5%ID within 50-80 min after injection. The greatest accumulation of 2-[^18^F]FA was in the thalamus, followed by the midbrain and pons. About 89-93% of ID was excreted in urine. The organ that received the highest absorbed dose equivalent was found to be the urinary bladder (180 µSv/MBq or 0.66 rem/mCi) and all other organs (<51 µSv/MBq or 0.19 rem/mCi). The effective dose equivalent was calculated as 45 µSv/MBq (0.17 rem/mCi). Bottlaender et al. (14) estimated effective dose equivalent to be 20 µSv/MBq (0.074 rem/mCi) in a study of three male healthy volunteers.

## NIH Support

Intramural Research Program

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Sullivan J.P., Donnelly-Roberts D., Briggs C.A., Anderson D.J., Gopalakrishnan M., Piattoni-Kaplan M., Campbell J.E., McKenna D.G., Molinari E., Hettinger A.M., Garvey D.S., Wasicak J.T., Holladay M.W., Williams M., Arneric S.P. (1996). A-85380 [3-(2(S)-azetidinylmethoxy) pyridine]: in vitro pharmacological properties of a novel, high affinity alpha 4 beta 2 nicotinic acetylcholine receptor ligand. Neuropharmacology.
5 Horti A.G., Scheffel U., Koren A.O., Ravert H.T., Mathews W.B., Musachio J.L., Finley P.A., London E.D., Dannals R.F. (1998). 2-[18F]Fluoro-A-85380, an in vivo tracer for the nicotinic acetylcholine receptors. Nucl Med Biol.
6 Doll F., Dolci L., Valette H., Hinnen F., Vaufrey F., Guenther I., Fuseau C., Coulon C., Bottlaender M., Crouzel C. (1999). Synthesis and nicotinic acetylcholine receptor in vivo binding properties of 2-fluoro-3-[2(S)-2-azetidinylmethoxy]pyridine: a new positron emission tomography ligand for nicotinic receptors. J Med Chem.
7 Schmaljohann J., Minnerop M., Karwath P., Gundisch D., Falkai P., Guhlke S., Wullner U. (2004). Imaging of central nAChReceptors with 2-[18F]F-A85380: optimized synthesis and in vitro evaluation in Alzheimer's disease. Appl Radiat Isot.
8 Chefer S.I., Horti A.G., Koren A.O., Gundisch D., Links J.M., Kurian V., Dannals R.F., Mukhin A.G., London E.D. (1999). 2-[18F]F-A-85380: a PET radioligand for alpha4beta2 nicotinic acetylcholine receptors. Neuroreport.
9 Vaupel D.B., Stein E.A., Mukhin A.G. (2007). Quantification of alpha4beta2* nicotinic receptors in the rat brain with microPET and 2-[18F]F-A-85380. Neuroimage.
10 Valette H., Bottlaender M., Dolle F., Guenther I., Fuseau C., Coulon C., Ottaviani M., Crouzel C. (1999). Imaging central nicotinic acetylcholine receptors in baboons with [18F]fluoro-A-85380. J Nucl Med.
11 Chefer S.I., London E.D., Koren A.O., Pavlova O.A., Kurian V., Kimes A.S., Horti A.G., Mukhin A.G. (2003). Graphical analysis of 2-[18F]FA binding to nicotinic acetylcholine receptors in rhesus monkey brain. Synapse.
12 Valette H., Bottlaender M., Dolle F., Coulon C., Ottaviani M., Syrota A. (2005). Acute effects of physostigmine and galantamine on the binding of [18F]fluoro-A-85380: a PET study in monkeys. Synapse.
13 Kimes A.S., Horti A.G., London E.D., Chefer S.I., Contoreggi C., Ernst M., Friello P., Koren A.O., Kurian V., Matochik J.A., Pavlova O., Vaupel D.B., Mukhin A.G. (2003). 2-[18F]F-A-85380: PET imaging of brain nicotinic acetylcholine receptors and whole body distribution in humans. Faseb J.
14 Bottlaender M., Valette H., Roumenov D., Dolle F., Coulon C., Ottaviani M., Hinnen F., Ricard M. (2003). Biodistribution and radiation dosimetry of 18F-fluoro-A-85380 in healthy volunteers. J Nucl Med.